# Quantum dot-prostate-specific membrane antigen antibody J591

Chemical name: | Quantum dot-prostate-specific membrane antigen antibody J591
Abbreviated name: | QD655-PMSA, QD655-J591
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), folate hydrolase
Target category: | Antibody-antigen binding
Method of detection: | Optical, near-infrared fluorescence (NIR)
Source of signal: | Quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-1000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals (4).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1-10 nm (5-7). They can be tuned to emit in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow and symmetric emission spectra with long, excited-state lifetimes, 20-50 ns, as compared with 1-10 ns of fluorescent dyes. They process good quantum yields of 40-90% and high extinction coefficients. They are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugations with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which were tested in vitro and in vivo (7-11). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are only limited studies of long-term toxicity of QDs in small animals (12-20). However, little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (21, 22). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents (23, 24). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (2). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (3). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (4). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (2). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody (^111^In-labeled Capromomab pendetide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Capromab111In) (^111^In-CYT-356)) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (5). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (6, 7). J591, a monoclonal antibody against the extracellular domain of PSMA (25), was conjugated to QD655 (QD655-J591) and accumulated in a human prostate cancer cell line in vitro and in nude mice (15).

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/books?term=PSMA%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/gene/2346)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/600934))
- Clinical trials (J591 (http://www.clinicaltrials.gov/ct2/results?term=J591))
- Drug information in FDA (J591 (http://google2.fda.gov/search?q=j591&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20synthesis)]

Core shell CdSe-ZnS QDs were coated with tri-n-octylphosphine oxide (TOPO), a triblock amphiphilic copolymer, and polyethylene glycol (PEG) (15). The bioconjugation efficiency of J591 using ethyl-3-dimethyl(aminopropyl)carbodiimide to the QD655 was 40-50%. The assembled QDs have a hydrodynamic radius of 10-15 nm, as measured by dynamic light scattering. Each QD655-J591 contains 200 TOPO molecules, 4 to 5 triblock copolymers, 5 to 6 PEG molecules, and 5 to 6 J592 antibody molecules, as estimated by fluorescence-tagged molecules. Transmission electron microscopy indicated that the QD655-J591 consisted of single particles with little aggregation. QD655-J591 emits light at the NIR fluorescence range of 655 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a K_d_ of 1.83 nM with ^131^I-labeled J591 and a B_max_ of 600,000-800,00 sites/cell in a saturation binding assay (25). Binding studies of QD655-J591 and QD655-PEG were performed using human prostate cancer cell lines C4-2 (PSMA positive, a subclone of LNCaP) and PC-3 (PSMA negative) (15). QD655-J591 but not QD655-PEG was shown to bind to C4-2 cells. No fluorescence was detected on the cell surface of PC-3 cells with QD655-J591. QD655-J591 binds specifically to C4-2 cells, given that PC-3 cells without PSMA showed no binding by QD655-J591.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20rodentia)]

Tumor imaging studies of QD655-J591 were evaluated in nude mice bearing a C4-2 subcutaneous xenograft model (15). Whole-body small animal images by reflectance planar fluorescence were obtained after injection of QD655-J591, QD655 coated with surface carboxylic acid groups (QD655-COOH), and QD655-PEG. Intense tumor signals were obtained with QD655-J591 (0.4 nmol/mouse) at 2 h after injection (active targeting by specific antibody-antigen recognition). Weak tumor fluorescence signals were obtained with QD655-PEG (6 nmol/mouse) at 6 h (passive targeting by enhanced vascular permeability of tumor). No tumor fluorescence signals were obtained with QD655-COOH (6 nmol/mouse) at 24 h. However, QD655-J591 has suboptimal tissue penetration and autofluorescence from the skin. No negative control (QD655 conjugated with nonspecific antibody) or blocking experiments (unconjugated J591) were performed in these studies.

The biodistribution of QD655-J591, QD655-PEG, and QD655-COOH was studied in C4-2 tumor-bearing mice by ex vivo tissue fluorescence intensity measurements (15). QD655-J591 uptake in tumors was high, followed to a lesser extent by QD65-PEG. The uptake of QD655-COOH in the tumor was not detectable. QD655-J591, QD655-PEG, and QD655-COOH were all markedly retained in the liver and spleen as nonspecific uptake by the reticuloendothelial system, with little or no accumulation in the brain, heart, kidney, or lung.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20human%20not%20animal%20not%20cell%20line)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
6 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
7 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
8 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
9 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
10 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
11 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
12 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
13 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
14 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
15 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
16 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
17 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
18 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
19 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
20 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
21 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
22 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
23 Nanus, D.M., M.I. Milowsky, L. Kostakoglu, P.M. Smith-Jones, S. Vallabahajosula, S.J. Goldsmith, and N.H. Bander, Clinical use of monoclonal antibody HuJ591 therapy: targeting prostate specific membrane antigen. J Urol, 2003170(6 Pt 2): p. S84-8; discussion S88-9.
24 Nargund V., Al Hashmi D., Kumar P., Gordon S., Otitie U., Ellison D., Carroll M., Baithun S., Britton K.E. (2005). Imaging with radiolabelled monoclonal antibody (MUJ591) to prostate-specific membrane antigen in staging of clinically localized prostatic carcinoma: comparison with clinical, surgical and histological staging. BJU Int.
25 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.